# 8-Cyclopentyl-3-(3-[^18^F]fluoropropyl)-1-propylxanthine

Chemical name: | 8-Cyclopentyl-3-(3-[^18^F]fluoropropyl)-1-propylxanthine
Abbreviated name: | [^18^F]CPFPX
Synonym:
Agent category: | Compound
Target: | Adenosine A_1_ receptor
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20CPFPX)]

Adenosine is an endogenous nucleoside, which modulates a number of physiological functions in the central nervous system (CNS) and in peripheral organs, such as the heart, kidney and muscle (1, 2). The effect is mediated by two major subtypes of receptors (A_1_ and A_2A_ receptors) and two minor subtypes (A_2B_ and A_3_). In the CNS, A_1_ receptors are present both pre- and postsynaptically in the hippocampus, cerebral cortex, thalamus, striatum, and cerebellum. A_2A_ receptors are highly concentrated and co-localized with dopamine D_1_ and D_2_ receptors in the striatum, nucleus accumbens, and olfactory tubercle. A_2A_ receptors are also present in the hippocampus and cortex. A_2B_ receptors are widely distributed but high in gastrointestinal tract. A_3_ receptors are also widely distributed but high in testis. A_1_ and A_3_ receptors mediate inhibition of adenylyl cyclase, whereas A_2A_ and A_2B_ receptors mediate stimulation. Changes in the adenosine functions are implicated in epilepsy, ischemic cerebral stroke, movement disorders, sleep disorders and psychiatric disorders (3-5).

A_1_ receptors have been studied in vivo by positron emission tomography (PET) using [1-methyl-^11^C]8-dicyclopropylmethyl-1-methyl-3-propylxanthine ([18F]CPFPX ), a methyl xanthine analog of KF15372 with selective A_1_ antagonistic activity (6). 8-Cyclopentyl-1,3-dipropylxanthine was reported to be a selective A1 receptor antagonist and its analog, 8-Cyclopentyl-3-(3-fluoropropyl)-1-propylxanthine (CPFPX) has been labeled with ^18^F as 8-Cyclopentyl-3-(3-[^18^F]fluoropropyl)-1-propylxanthine ([^18^F]CPFPX). [^18^F]CPFPX is being developed as a PET agent for the non-invasive study of the human brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20CPFPX%20and%20synthesis)]

In the report by Noguchi et al., [18F]CPFPX was synthesized by alkylation of the 1-N-desmethyl precursor (8-dicyclopropylmethyl-3-propylxanthine) with [^11^C]methyl iodide in the presence of NaH, with subsequent purification by high-performance liquid chromatography. Radiochemical purity was greater than 98%. The average specific activity was 49 GBq/μmol (1.3 Ci/μmol) at the end of synthesis. Total synthesis time was 45-60 min.

Kawamura et al. described the synthesis of [^18^F]CPFPX from the desmethyl precursor with [^11^C]methyl triflate in the presence of Cs_2_CO_3_ providing an improved radiochemical yield of 55.3% based on [^11^C]methyl triflate. No time of synthesis and specific activity were reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20CPFPX%20and%20in%20vitro)]

The K_i_ values of MPDX and KF15372 for the A_1_ receptors were 4.2 nM and 3.0 nM, respectively. The K_i_ values for both antagonists for A_2A_ receptors were >100 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20CPFPX%20and%20rodentia)]

Biodistribution studies in normal mice showed high accumulation of radioactivity in the liver (8.5% injected dose (ID)/g), followed by the small intestine (3.8% ID/g), pancreas (3.2% ID/g), kidney (2.3% ID/g), and spleen (1.9% ID/g) at 30 min after injection of [18F]CPFPX . The level of radioactivity was low in the brain (0.7% ID/g) and blood (1.5% ID/g). Coadiministration of the A_1_ antagonist KF15372 but not A_2A_ antagonist KF17837 decreased the accumulation in the brain in a dose-dependent manner at 15 min post injection. About 22-27% and 62-65% of radioactivity in the plasma and cerebral cortex was intact [18F]CPFPXat 30 min post injection, respectively.

Kiyosawa et al. studied the changes in the distribution of central benzodiazepine and presynaptic A_1_ receptors in the superior colliculus (SC) and visual cortex (VC) of rats following monocular enucleation. The uptake of [^14^C]deoxyglucose in the SC was depressed immediately after enucleation and gradually recovered. The binding of [^11^C]flumazenil to central benzodiazepine receptors in the contralateral SC was increased at week 2, and then returned to the pre-enucleation levels. The uptake of [18F]CPFPXby the A_1_ receptors in the contralateral SC decreased by about 67% on day 5 after enucleation and remained low thereafter. In the contralateral VC, the uptake of [^14^C]deoxyglucose decreased immediately after the enucleation followed by a gradual recovery, whereas the uptake of [^11^C]flumazenil and [18F]CPFPXwas not affected. The axon degeneration decreased the A_1_ receptor density and resulted in a transient increase of postsynaptic central benzodiazepine receptor density in the enucleated rats.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20CPFPX%20and%20%28dog%20or%20cat%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Shimadaet al. obtained PET images of the brain in cats after injection of 199 MBq (5.4 mCi) [18F]CPFPX . Regional brain distribution and kinetics of [18F]CPFPXwere studied with MRI co-registration. The cerebral cortex exhibited the highest accumulation of [18F]CPFPX(distribution volume, DV = 4.2 ± 1.7) followed by the striatum (DV = 3.8 ± 1.3), cerebellum (DV = 3.5 ± 1.2), thalamus (DV = 3.1 ± 1.2), midbrain (DV = 2.6 ± 0.9) and whole brain (DV = 2.4 ± 0.8). Co-injection with unlabeled MDPX inhibit binding of [18F]CPFPXto the regional brain areas.

Nariai et al. studied the adenosine A_1_ receptor with PET using [18F]CPFPXin a cat cerebral ischemic model (middle cerebral artery occlusion and reperfusion). Eighteen adult cats underwent PET measurement of cerebral blood flow (CBF) with ^15^O-labeled water, A_1_ receptors with [18F]CPFPX , central benzodiazepine receptors with [^11^C]flumazenil and glucose metabolism with [^18^F]fluorodeoxyglucose (FDG) after 60 min occlusion. [18F]CPFPXbinding and [^11^C]flumazenil binding, but not CBF and FDG uptake, were significantly reduced in the groups with severer ischemic insult than in the groups with no or milder insults. Of the two receptor ligands, the reduction rate of the [18F]CPFPXbinding to A_1_ receptors was larger in a group that caused fatal ischemic insult. Therefore, [18F]CPFPXPET imaging was suitable in evaluating the function of adenosine A_1_ receptors in relation to cerebral ischemia.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20CPFPX%20and%20%28primate%20not%20human%29)]

Using PET, Ishiwata et al. obtained serial brain scans in 2 monkeys after injection of 91-141 MBq (2.5-3.8 mCi) [18F]CPFPX . The accumulation of radioactivity in the brain peaked at 5 min, and then decreased for the final 60 min of study. The fraction of unchanged [18F]CPFPXin blood samples determined by HPLC was 78%, 70%, 54% and 41% at 5, 15, 30 and 60 min, respectively.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20CPFPX%20and%20human)]

Kimura et al. reported on PET studies in 7 healthy volunteers after injection of 259-777 MBq (7-21 mCi) of [18F]CPFPX . Using Logan plot analysis, the striatum (0.55) exhibited the highest binding potential (BP, cerebellum as a reference) for [18F]CPFPX , followed by thalamus (0.50), occipital cortex (0.40), parietal cortex (0.33) and temporal cortex (0.28). Fukumitsu et al. extended the human PET studies using Logan plot analysis with arterial input. The DV was large in the striatum and thalamus, moderate in the cerebral cortices and small in the cerebellum. The distribution of pattern of [18F]CPFPXin the brain was discretely different from that of CBF as measured by ^15^O-labeled water. At 60 min after injection of [18F]CPFPX , 75% of radioactivity was in the intact tracer. This percentage was much higher than those in rats (22-27%), cats (6.5%) and monkeys (41%). Naganawa et al. reported that DV and BP could be accurately estimated without arterial blood sampling in 25 subjects. Internal dosimetry data for [18F]CPFPXin humans are not available in the literature.

## References

1 Fredholm B.B., Abbracchio M.P., Burnstock G., Daly J.W., Harden T.K., Jacobson K.A., Leff P., Williams M. (1994). Nomenclature and classification of purinoceptors. Pharmacol Rev.
2 Palmer T.M., Stiles G.L. (1995). Adenosine receptors. Neuropharmacology.
3 Dunwiddie T.V., Masino S.A. (2001). The role and regulation of adenosine in the central nervous system. Annu Rev Neurosci.
4 El Yacoubi M., Costentin J., Vaugeois J.M. (2003). Adenosine A2A receptors and depression. Neurology.
5 von Lubitz D.K. (2001). Adenosine in the treatment of stroke: yes, maybe, or absolutely not?. Expert Opin Investig Drugs.
6 Shimada J., Suzuki F., Nonaka H., Karasawa A., Mizumoto H., Ohno T., Kubo K., Ishii A. (1991). 8-(Dicyclopropylmethyl)-1,3-dipropylxanthine: a potent and selective adenosine A1 antagonist with renal protective and diuretic activities. J Med Chem.
7 Noguchi J., Ishiwata K., Furuta R., Simada J., Kiyosawa M., Ishii S., Endo K., Suzuki F., Senda M. (1997). Evaluation of carbon-11 labeled KF15372 and its ethyl and methyl derivatives as a potential CNS adenosine A1 receptor ligand. Nucl Med Biol.
8 Kawamura K., Ishiwata K. (2004). Improved synthesis of [11C]SA4503, [18F]CPFPXand [11C]TMSX by use of [11C]methyl triflate. Ann Nucl Med.
9 Kiyosawa M., Ishiwata K., Noguchi J., Endo K., Wang W.F., Suzuki F., Senda M. (2001). Neuroreceptor bindings and synaptic activity in visual system of monocularly enucleated rat. Jpn J Ophthalmol.
10 Nariai T., Shimada Y., Ishiwata K., Nagaoka T., Shimada J., Kuroiwa T., Ono K., Ohno K., Hirakawa K., Senda M. (2003). PET imaging of adenosine A(1) receptors with (11)C-MPDX as an indicator of severe cerebral ischemic insult. J Nucl Med.
11 Nariai T., Shimada Y., Ishiwata K., Nagaoka T., Shimada J., Kuroiwa T., Ono K.I., Hirakawa K., Senda M., Ohno K. (2003). PET neuroreceptor imaging as predictor of severe cerebral ischemic insult. Acta Neurochir Suppl.
12 Ishiwata K., Nariai T., Kimura Y., Oda K., Kawamura K., Ishii K., Senda M., Wakabayashi S., Shimada J. (2002). Preclinical studies on [18F]CPFPXfor mapping adenosine A1 receptors by positron emission tomography. Ann Nucl Med.
13 Kimura Y., Ishii K., Fukumitsu N., Oda K., Sasaki T., Kawamura K., Ishiwata K. (2004). Quantitative analysis of adenosine A1 receptors in human brain using positron emission tomography and [1-methyl-11C]8-dicyclopropylmethyl-1-methyl-3-propylxanthine. Nucl Med Biol.
14 Fukumitsu N., Ishii K., Kimura Y., Oda K., Sasaki T., Mori Y., Ishiwata K. (2005). Adenosine A1 receptor mapping of the human brain by PET with 8-dicyclopropylmethyl-1-11C-methyl-3-propylxanthine. J Nucl Med.
15 Fukumitsu N., Ishii K., Kimura Y., Oda K., Sasaki T., Mori Y., Ishiwata K. (2003). Imaging of adenosine A1 receptors in the human brain by positron emission tomography with [18F]CPFPX . Ann Nucl Med.
16 Naganawa M., Kimura Y., Nariai T., Ishii K., Oda K., Manabe Y., Chihara K., Ishiwata K. (2005). Omission of serial arterial blood sampling in neuroreceptor imaging with independent component analysis. Neuroimage.